# 1-(5-[^18^F]Fluoro-5-deoxy-α-D-arabinofuranosyl)-2-nitroimidazole

Chemical name: | 1-(5-[^18^F]Fluoro-5-deoxy-α-D-arabinofuranosyl)-2-nitroimidazole
Abbreviated name: | [^18^F]FAZA
Synonym: | [^18^F]Fluoroazomycinarabinofuranoside, [^18^F]Fluoroazomycin arabinoside,
Agent Category: | Compound
Target: | Hypoxic tissue
Target Category: | Intracellular reduction and binding to macromolecules
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20and%20FAZA)]

Hypoxia was found in a variety of solid tumors, leading to tumor progression and the resistance of tumors to chemotherapy and radiotherapy (1-3). Tumor oxygenation is heterogeneously distributed within human tumors (4). It would be beneficial to assess tumor oxygenation before and after therapy to provide an evaluation of tumor response to treatment and an insight into new therapeutic treatments (5). Tumor oxygenation is measured invasively using computerized polarographic oxygen-sensitive electrodes, which is regarded as the gold standard (6). Functional and non-invasive imaging of intratumoral hypoxia has been demonstrated to be feasible for the measurement of tumor oxygenation (7).

Chapman proposed the use of 2-nitroimidazoles for hypoxia imaging in 1979 (8). 2-Nitroimidazole compounds are postulated to undergo reduction in hypoxic condition, forming highly reactive oxygen radicals that subsequently bind covalently to macromolecules inside the cells (9). [^18^F]Fluoromisonidazole ([^18^F]FMISO) is the most widely used positron emission tomography (PE) tracer for imaging tumor hypoxia (7). However, it has slow clearance kinetics and a high lipophilicity, resulting in substantially high background in PET scan. [^18^F]Fluoroazomycinarabinofuranoside ([^18^F]FAZA) is a 2-nitroimidazole with a sugar addition (10). [^18^F]FAZA was studied as hypoxia imaging agent, showing promising results in various tumor models in rats and mice (11, 12). [^18^F]FAZA PET imaging of tumour hypoxia was evaluated in patients with squamous cell carcinoma of the head and neck (HNSCC), small-cell lung cancer (SCLC) or non-small-cell lung cancer (NSCLC), malignant lymphoma, and high-grade gliomas (13, 14).

### Related Resource Links:

- Chapters in MICAD (Hypoxia (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=Hypoxia+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (Hypoxia (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=3091))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Hypoxia (http://www.ncbi.nlm.nih.gov/omim?Db=omim&Cmd=DetailsSearch&Term=hypoxia%5BAll+Fields%5D))
- Clinical trials ([^18^F]FAZA (http://www.clinicaltrials.gov/ct2/results?term=FAZA&Search=Search))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2818F%20and%20FAZA%29%20and%20synthesis)]

[^18^F]FAZA was readily synthesized by standard nucleophilic substitution conditions (Kryptofix 2.2.2 and K_2_CO_3_), followed by hydrolysis of the protective acetyl groups using 1-(2,3-di-O-acetyl-5-O-tosyl-α-D-arabinofuranosyl)-2-nitroimidazole and [^18^F]fluoride (12). Radiochemical yield averaged 20% (decay corrected) based on [^18^F]fluoride, and the specific activity averaged 2 GBq/μmol (54 mCi/μmol) at the end of synthesis. Radiochemical and chemical purities were 90-95% as determined by high-performance liquid chromatography (HPLC). Reisch et al. (10) used an automated synthesis to provide an overall radiochemical yield of 20.7 ± 3.5% (not decay corrected) and absolute yields up to 9.8 ± 2.3 GBq (260 ± 62 mCi) at the end of synthesis. The synthesis time was 50 min.

In comparison studies, [^18^F]FMISO was synthesized using 1-(2-nitro-1-imidazolyl)-2-O-tetrahydropyranyl-3-O-toluene-sulfonylpropane-diol by nucleophilic substitution with [^18^F]fluoride, followed by hydrolysis (12). This provided [^18^F]FMISO in 80% (decay corrected) radiochemical yield and 90-95% radiochemical purity at the end of synthesis with a specific activity of 2 GBq/μmol (54 mCi/μmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20and%20FAZA%20and%20in%20vitro)]

In vitro studies (12) indicated that uptake of both [^18^F]FAZA and [^18^F]FMISO in Walker 256 rat tumor cells in hypoxic culture condition (pO_2_ < 3 mm Hg) in 20 and 100 min of incubation was of the same magnitude (20 min: 1.24 ± 0.4% ([^18^F]FAZA); 1.19 ± 0.7% ([^18^F]FMISO); 100 min: 3.6 ± 1.6% ([^18^F]FAZA); 3.3 ± 1.7% ([^18^F]FMISO)). Under normoxic culture condition (pO_2_, 70 mm Hg), their uptake was similar but lower than in the hypoxic condition (20 min: 0.9 ± 0.4% ([^18^F]FAZA); 0.74 ± 0.3% ([^18^F]FMISO); 100 min: 1.1 ± 0.6% ([^18^F]FAZA); 1.4 ± 0.6% ([^18^F]FMISO)).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20and%20FAZA%20and%20rodentia)]

Standardized uptake values (SUVs, Bq per cm^3^ X body weight in g divided by injected dose) for [^18^F]FAZA and [^18^F]FMISO were determined with PET scan in rats bearing Walker 256 carcinosarcoma in their right hind legs (12). Tissue pO_2_ values of the normal muscle and tumors were 50-70 and <5 mm Hg, respectively. One h after tracer injection, the SUVs in tumors were 0.68 ± 0.2 for [^18^F]FAZA and 1.07 ± 0.3 for [^18^F]FMISO (p < 0.05). Corresponding SUVs in muscle tissue were 0.29 ± 0.09 for [^18^F]FAZA and 0.40 ± 0.09 for [^18^F]FMISO (p < 0.05). The concentration of [^18^F]FAZA in tumor and muscle tissue at 3 h after tracer injection was concordantly decreased to SUVs of 0.35 ± 0.12 (tumor) and 0.13 ± 0.05 (muscle). However, the SUV for [^18^F]FMISO in the tumor tissue remained unchanged in 3-h PET imaging (1.11 ± 0.7), although it was lower in comparison with early PET scans for the muscle tissue (0.26 ± 0.15). Tumor-to-muscle SUV ratio was not significantly different ([^18^F]FAZA, 2.4 ± 0.6; [^18^F]FMISO, 2.7 ± 0.6) when measured 1 h after injection. However, the tumor-to-muscle ratio was significantly higher for [^18^F]FMISO in comparison with [^18^F]FAZA (4.4 ± 1.3 versus 2.9 ± 0.6, p < 0.05) at 3 h. PET images showed that [^18^F]FAZA radioactivity was eliminated via the renal system with high radioactivity in the kidneys and urinary bladder and low radioactivity in the liver. In contrast, [^18^F]FMISO was high in the kidneys and liver. [^18^F]FAZA showed a faster clearance from the body than [^18^F]FMISO, providing a lower background than [^18^F]FMISO.

Biodistribution studies (11) of [^18^F]FAZA in nude mice bearing AR42J tumors showed a rapid clearance of the tracer from the body over time (10, 60, and 180 min after injection). The highest decrease in radioactivity was found in the blood and the lowest decrease was found in tumor and brain. The tumor-to-muscle ratio increased with time. [^18^F]FAZA was eliminated via renal excretion and hepatic metabolism as the radioactivity in the liver and kidneys also decreased from 10 to 180 min. The highest radioactivity was found in the urine (100%ID/g urine) followed by the tumor, intestines, kidneys, and liver at 180 min.

[^18^F]FAZA and [^18^F]FMISO biodistribution studies were compared in the three different tumor models (EMT6 BALB/c mice, AR42J and A431 Swiss nude mice) at 3 h after tracer injection (11). [^18^F]FAZA exhibited a significantly lower uptake in most organs, including the liver and kidneys, and a much faster clearance from the blood compared with [^18^F]FMISO. In contrast, tumor uptake was not significantly different between both tracers in two of the three tumor models studied. However, [^18^F]FAZA showed a more favorable tumor-to-blood ratio and tumor-to-organ ratios than [^18^F]FMISO. Tumor hypoxia was assessed in EMT6 (pO_2_, 2.9 ± 2.6) and AR42J (pO_2_, 0.4 ± 0.2) by oxygen electrode measurements as compared with normal tissue (pO_2_, 25.8-29.0). Therefore, tumor uptake of [^18^F]FAZA correlates inversely with oxygen concentration.

Serial animal [^18^F]FAZA PET studies (11) were performed in nude mice bearing A431 tumors and showed that the tumor-to-background ratio was significantly higher in mice breathing room air compared with that of mice breathing pure oxygen (7.3 ± 2.3 versus. 4.2 ± 1.2, respectively; p < 0.001). Similarly, autoradiography studies in mice bearing EMT6 tumor showed significantly higher tumor-to-muscle ratios in mice breathing room air compared with those of animals breathing carbogen (95% O_2_ and 5% CO_2_) (5.3 ± 0.8 versus 2.2 ± 0.8; respectively; p < 0.02). Hence, uptake of [^18^F]FAZA would be decreased by improving tumor tissue oxygenation through therapy.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20and%20FAZA%20and%20%28dog%20or%20pig%20or%20cat%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20and%20FAZA%20and%20primate%20not%20human)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20and%20FAZA%20and%20humans)]

Souvatzoglou et al. (13) reported [^18^F]FAZA PET studies in 11 patients (age 45-75 yr) with squamous cell carcinoma of the head and neck (HNSCC). Dynamic scanning was performed for 2 h after intravenous injection of 315 ± 91 MBq (8.5 ± 2.5 mCi) [^18^F]FAZA with a whole-body static scan performed at 2 h. Within the first 60 min of the dynamic scanning, the tumor/muscle ratio generally decreased, while generally increasing at later time points. At 2 h , the tumour SUV(max) and SUV(mean) were found to be 2.3 ± 0.5 (range 1.5-3.4) and 1.4 ± 0.3 (range 1.0-2.1), respectively. The mean tumor/muscle ratio at 2 h was 2.0 ± 0.3 (range 1.6-2.4). The tumour volume displaying a tumor/muscle ratio above 1.5 was highly variable. At 2 h, organ radioactivity distribution order was determined as follows: kidney > gallbladder > liver > tumour > muscle > bone > brain > lung.

Postema et al. (14) reported [^18^F]FAZA PET studies in 50 patients (age 18-90 yr) with HNSCC (n = 9), small-cell lung cancer (SCLC) (n = 1), non-small-cell lung cancer (NSCLC) (n = 12), malignant lymphoma (n = 21), or high-grade gliomas (n = 7). Dynamic scanning was performed for 2-3 h after intravenous injection of 338-682 MBq (9.1-18.4 mCi) [^18^F]FAZA. All seven patients with high-grade gliomas showed very high uptake of [^18^F]FAZA (average tumor/blood ratio, 5.3) in the primary tumour. In six out of nine patients with HNSCC, clear uptake of [^18^F]FAZA (average tumor/blood ratio, 2.0) was observed in the primary tumour and/or the lymph nodes in the neck. Of the 21 lymphoma patients, 3 demonstrated moderate lymphoma-related [^18^F]FAZA uptake (average tumor/blood ratio, 2.2). Of the 13 lung cancer patients, 7 patients had increased [^18^F]FAZA uptake (average tumor/blood ratio, 2.5) in the primary lung tumour. No side effects of the administration of [^18^F]FAZA were observed. The investigators concluded that [^18^F]FAZA may be a very useful tracerl for imaging hypoxia in these tumour types.

## References

1 Rajendran J.G., Krohn K.A. (2005). Imaging hypoxia and angiogenesis in tumors. Radiol Clin North Am.
2 Serkies K., Jassem J. (2005). Chemotherapy in the primary treatment of cervical carcinoma. Crit Rev Oncol Hematol.
3 Vaupel P., Mayer A. (2005). Hypoxia and anemia: effects on tumor biology and treatment resistance. Transfus Clin Biol.
4 Vaupel P., Harrison L. (2004). Tumor hypoxia: causative factors, compensatory mechanisms, and cellular response. Oncologist.
5 Dehdashti F., Grigsby P.W., Mintun M.A., Lewis J.S., Siegel B.A., Welch M.J. (2003). Assessing tumor hypoxia in cervical cancer by positron emission tomography with 60Cu-ATSM: relationship to therapeutic response-a preliminary report. Int J Radiat Oncol Biol Phys.
6 Raleigh J.A., Dewhirst M.W., Thrall D.E. (1996). Measuring Tumor Hypoxia. Semin Radiat Oncol.
7 Foo S.S., Abbott D.F., Lawrentschuk N., Scott A.M. (2004). Functional imaging of intratumoral hypoxia. Mol Imaging Biol.
8 Chapman J.D. (1979). Hypoxic sensitizers--implications for radiation therapy. N Engl J Med.
9 Chapman J.D., Baer K., Lee J. (1983). Characteristics of the metabolism-induced binding of misonidazole to hypoxic mammalian cells. Cancer Res.
10 Reischl G., Ehrlichmann W., Bieg C., Solbach C., Kumar P., Wiebe L.I., Machulla H.J. (2005). Preparation of the hypoxia imaging PET tracer [18F]FAZA: reaction parameters and automation. Appl Radiat Isot.
11 Piert M., Machulla H.J., Picchio M., Reischl G., Ziegler S., Kumar P., Wester H.J., Beck R., McEwan A.J., Wiebe L.I., Schwaiger M. (2005). Hypoxia-specific tumor imaging with 18F-fluoroazomycin arabinoside. J Nucl Med.
12 Sorger D., Patt M., Kumar P., Wiebe L.I., Barthel H., Seese A., Dannenberg C., Tannapfel A., Kluge R., Sabri O. (2003). [18F]Fluoroazomycinarabinofuranoside (18FAZA) and [18F]Fluoromisonidazole (18FMISO): a comparative study of their selective uptake in hypoxic cells and PET imaging in experimental rat tumors. Nucl Med Biol.
13 Souvatzoglou M., Grosu A.L., Roper B., Krause B.J., Beck R., Reischl G., Picchio M., Machulla H.J., Wester H.J., Piert M. (2007). Tumour hypoxia imaging with [18F]FAZA PET in head and neck cancer patients: a pilot study. Eur J Nucl Med Mol Imaging.
14 Postema E.J., McEwan A.J., Riauka T.A., Kumar P., Richmond D.A., Abrams D.N., Wiebe L.I. (2009). Initial results of hypoxia imaging using 1-alpha-D: -(5-deoxy-5-[18F]-fluoroarabinofuranosyl)-2-nitroimidazole (18F-FAZA). Eur J Nucl Med Mol Imaging.